# (20R)-4,5-α-Epoxy-17-methyl-3-hydroxy-6-[^11^C]methoxy-α,17-dimethyl-α-(2-phenylethyl)-6,14-ethenomorphinan-7-methanol

Chemical name: | (20R)-4,5-α-Epoxy-17-methyl-3-hydroxy-6-[^11^C]methoxy-α,17-dimethyl-α-(2-phenylethyl)-6,14-ethenomorphinan-7-methanol
Abbreviated name: | [^11^C]PEO, [6-O-methyl-^11^C]PEO
Synonym: | [6-O-methyl-^11^C](20R)-Phenylethyl orvinol
Agent category: | Compound
Target: | Opioid receptors
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal\contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20PEO)]

Opioids such as morphine are analgesics that are commonly used in clinical practice. Three opioid receptors (mu, µ; delta, δ; and kappa, κ) that mediate opioid effects have been identified by molecular cloning: δ (enkephalin-preferring), κ (dynorphin-preferring), and µ (morphine- and ß-endorphin–preferring) (1). Each type of opioid receptors consists of subtypes of receptors as suggested by pharmacological studies (2, 3). These receptors exhibit apparent specificity to both the central and peripheral nervous systems, and their presence is ubiquitous in these systems. The opioid receptors (G-protein–coupled, resulting in decrease in adenylyl cyclase activity) play an important role in the regulation of analgesia, shock, appetite, thermoregulation, and cardiovascular, mental, and endocrine function (2-5). Although µ opioid receptors are the major receptors to mediate the analgesic effects of opioids, δ and κ receptors are also important in antinociception. Opioids have been found to protect cells from ischemic injury in the heart and brain via the δ receptors. On the other hand, κ antagonists prevent neurodegeneration.

The µ opioid receptors are localized predominately in the hypothalamus and thalamus, and the δ opioid receptors are localized predominately in the striatum, limbic system, and cerebral cortex (6, 7). The κ opioid receptors (κ_1_ and κ_2_) are the most abundant brain opioid receptors and are widely distributed in deeper layers of the neocortex (particularly temporal, parietal, and frontal cortices), striatum, amygdala, and thalamus, with lower levels in the hippocampus, occipital cortex, and cerebellum (8-10). The κ opioid receptors have been implicated in several clinical brain disorders, including drug abuse (11), epilepsy (12), Tourette’s syndrome (13), and Alzheimer’s disease (14).

Diprenorphine is a highly potent and nonselective opioid receptor antagonist with subnanomolar affinity (7). Diprenorphine has been labeled as [6-O-methyl-^11^C]diprenorphine ([^11^C]DPN) (15, 16). [^11^C]DPN is being developed as a positron emission tomography (PET) agent for the non-invasive study of opioid receptors in the brain. However, pharmacological studies in humans (17) and rats (18) demonstrated minimal competition between the high-efficacy agonists and the non-subtype–selective antagonist radioligand [^11^C]DPN, which limits the use of [^11^C]DPN PET to monitor in vivo occupancy. (20R)-4,5-α-Epoxy-17-methyl-3-hydroxy-6-methoxy-α,17-dimethyl-α-(2-phenylethyl)-6,14-ethenomorphinan-7-methanol (PEO) was found to be a highly potent opioid receptor agonist (19). [6-O-methyl-^11^C]PEO ([^11^C]PEO) has been evaluated for PET imaging of opioid receptors in rats.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Opioid+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20PEO%20and%20synthesis)]

Marton et al. (19) performed synthesis of [^11^C]PEO by [^11^C]-O-methylation of the trityl-protected precursor (2.85 µmol) with [^11^C]methyl iodide for 5 min at 90ºC. Final acidic deprotection of the product was performed in an automatic synthesis module. An average radiochemical yield was 57 ± 16% (n = 16, decay-corrected) with a total synthesis time of ~30 min. Average specific activity was 60 GBq/μmol (1.62 Ci/μmol) at end of synthesis with a radiochemical purity of >99%. The log P of [^11^C]PEO was 2.36.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20PEO%20and%20in%20vitro)]

Marton et al. (19) reported in vitro binding assays using membranes of human cloned receptor stably expressed on Chinese hamster ovary (CHO) cells (µ and κ) and HEK-293 cells (δ). PEO had inhibition constant (K_i_) values of 0.18, 0.12, and 5.1 nM for the µ ([^3^H]DPN), κ ([^3^H]DPN), and δ ([^3^H]naltrindole) opioid receptors, respectively. Therefore, PEO binds to µ and κ, subtypes of opioid receptors with higher affinity than the δ subtype. The agonist efficacy of PEO was 105% relative to full effect of DAMGO (µ-agonist) and 113% relative to that of U69593 (κ-agonist).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20PEO%20and%20rodentia)]

Marton et al. performed biodistribution studies in rats injected with 24 MBq (0.65 mCi) [^11^C]PEO (19), which showed high accumulation of radioactivity in the striatum (0.89% injected dose/gram (ID/g)), thalamus (0.78% ID/g), and frontal cortex (0.76% ID/g) at 60 min after injection. Brain regions to cerebellum ratios increased over time with ratios of 2.95–3.78 at 20 min and of 4.47–5.23 at 60 min. Pretreatment with cyprodime (µ antagonist) decreased the radioactivity levels by 82–86% in the striatum, thalamus, and frontal cortex. Furthermore, pretreatment with naloxone (an opioid receptor antagonist) decreased the radioactivity levels by >95% in the striatum, thalamus, and frontal cortex. The fraction of unchanged [^11^C]PEO in the brain determined with high-performance liquid chromatography was >92% at 40 min after injection. PET imaging showed high standardized uptake value (SUV) in the basal ganglia (1.0) and frontal cortex (1.0) and low SUV in the cerebellum (0.2) at 60 min after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20PEO%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20PEO%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20PEO%20and%20human)]

No publication is currently available.

## References

1 Minami M., Satoh M. (1995). Molecular biology of the opioid receptors: structures, functions and distributions. Neurosci Res.
2 Waldhoer M., Bartlett S.E., Whistler J.L. (2004). Opioid receptors. Annu Rev Biochem.
3 Satoh M., Minami M. (1995). Molecular pharmacology of the opioid receptors. Pharmacol Ther.
4 Molina P.E. (2006). Opioids and opiates: analgesia with cardiovascular, haemodynamic and immune implications in critical illness. J Intern Med.
5 Barry U., Zuo Z. (2005). Opioids: old drugs for potential new applications. Curr Pharm Des.
6 Chang K.J., Cooper B.R., Hazum E., Cuatrecasas P. (1979). Multiple opiate receptors: different regional distribution in the brain and differential binding of opiates and opioid peptides. Mol Pharmacol.
7 Pfeiffer A., Pasi A., Mehraein P., Herz A. (1982). Opiate receptor binding sites in human brain. Brain Res.
8 Peckys D., Landwehrmeyer G.B. (1999). Expression of mu, kappa, and delta opioid receptor messenger RNA in the human CNS: a 33P in situ hybridization study. Neuroscience.
9 Hiller J.M., Fan L.Q. (1996). Laminar distribution of the multiple opioid receptors in the human cerebral cortex. Neurochem Res.
10 Simonin F., Gaveriaux-Ruff C., Befort K., Matthes H., Lannes B., Micheletti G., Mattei M.G., Charron G., Bloch B., Kieffer B. (1995). kappa-Opioid receptor in humans: cDNA and genomic cloning, chromosomal assignment, functional expression, pharmacology, and expression pattern in the central nervous system. Proc Natl Acad Sci U S A.
11 Mello N.K., Negus S.S. (2000). Interactions between kappa opioid agonists and cocaine. Preclinical studies. Ann N Y Acad Sci.
12 de Lanerolle N.C., Williamson A., Meredith C., Kim J.H., Tabuteau H., Spencer D.D., Brines M.L. (1997). Dynorphin and the kappa 1 ligand [3H]U69,593 binding in the human epileptogenic hippocampus. Epilepsy Res.
13 Chappell P.B., Leckman J.F., Scahill L.D., Hardin M.T., Anderson G., Cohen D.J. (1993). Neuroendocrine and behavioral effects of the selective kappa agonist spiradoline in Tourette's syndrome: a pilot study. Psychiatry Res.
14 Mathieu-Kia A.M., Fan L.Q., Kreek M.J., Simon E.J., Hiller J.M. (2001). Mu-, delta- and kappa-opioid receptor populations are differentially altered in distinct areas of postmortem brains of Alzheimer's disease patients. Brain Res.
15 Lever J.R., Dannals R.F., Wilson A.A., Ravert H.T., Wagner H.N. (1987). Synthesis of carbon-11 labeled diprenorphine: a radioligand for positron emission tomographic studies of opiate receptors. Tetrahedron Letters.
16 Luthra S.K., Brady F., Turton D.R., Brown D.J., Dowsett K., Waters S.L., Jones A.K., Mathews R.W., Crowder J.C. (1994). Automated radiosyntheses of [6-O-methyl-11C]diprenorphine and [6-O-methyl-11C]buprenorphine from 3-O-trityl protected precursors. Appl Radiat Isot.
17 Melichar J.K., Hume S.P., Williams T.M., Daglish M.R., Taylor L.G., Ahmad R., Malizia A.L., Brooks D.J., Myles J.S., Lingford-Hughes A., Nutt D.J. (2005). Using [11C]diprenorphine to image opioid receptor occupancy by methadone in opioid addiction: clinical and preclinical studies. J Pharmacol Exp Ther.
18 Hume S.P., Lingford-Hughes A.R., Nataf V., Hirani E., Ahmad R., Davies A.N., Nutt D.J. (2007). Low sensitivity of the positron emission tomography ligand [11C]diprenorphine to agonist opiates. J Pharmacol Exp Ther.
19 Marton J., Schoultz B.W., Hjornevik T., Drzezga A., Yousefi B.H., Wester H.J., Willoch F., Henriksen G. (2009). Synthesis and evaluation of a full-agonist orvinol for PET-imaging of opioid receptors: [11C]PEO. J Med Chem.